# syn-1-Amino-3-[^18^F]fluorocyclobutane-1-carboxylic acid

Chemical name: | syn-1-Amino-3-[^18^F]fluorocyclobutane-1-carboxylic acid
Abbreviated name: | syn-3-[^18^F]FACBC, syn-[^18^F]FACBC
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facbc%5BAll%20Fields%5D)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain tissue (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine, and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used in imaging in oncology (4-6). The natural amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and retained in tumor cells because of their higher than normal metabolic pathways, including incorporation into proteins (4). L-[^11^C]Methionine and [^18^F]fluorotyrosine have been widely used in the detection of tumors although neither are approved by the FDA. On the other hand, the non-natural amino acids are not metabolized but are taken up through both the L-type transporter and the energy-dependent A-type transporter (7). Therefore, they can accumulate intracellularly in high concentrations. anti-1-Amino-3-[^18^F]fluorocyclobutane-1-carboxylic acid (anti-[^18^F]FACBC (http://www.ncbi.nlm.nih.gov/books/NBK23315/#FACBC18F)) was shown to have a high tumor/brain ratio (8), and anti-[^18^F]FACBC has been studied in humans with PET tumor imaging (9). In this chapter, syn-1-Amino-3-[^18^F]fluorocyclobutane-1-carboxylic acid (syn-3-[^18^F]FACBC) has also been synthesized and studied as a potential PET brain tumor imaging agent (10).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D)
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+synthesis)]

Nucleophilic fluorination of anti-1-[N-(phthaloyl)amino]-3-trifluoromethanesulfonoxy-1-cyclobutane-1-carboxylic acid methyl ester with K[^18^F]F/Kryptofix2.2.2 and subsequent acidic hydrolysis and purification provided a radiosynthesis yield of 51.5 ± 15.6% (decay-corrected, n = 7) of syn-3-[^18^F]FACBC at the end of bombardment (EOB) (10). A radiochemical purity of >95% was obtained. The total synthesis time was ~80 min from EOB. The specific activity of syn-3-[^18^F]FACBC was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+in+vitro)]

syn-3-[^18^F]FACBC exhibited rapid uptake into rat 9L gliosarcoma tumor cells in culture with 15.8 ± 2.4% injected dose (ID)/5 × 10^5^ cells (n = 3) at 30 min of incubation (10). The uptake was reduced by 38.6% and 77.8% by the presence of 10 mM 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (BCH, L-type transporter inhibitor) and a mixture of alanine, cysteine, and serine (ACS), respectively. N-methyl-α-aminoisobutyric acid (MeAIB, A-type transporter inhibitor) exhibited little inhibition. In comparison, anti-3-[^18^F]FACBC uptake into rat 9L gliosarcoma tumor cells in culture was reduced by 76%, 6%, and 98% by the presence of 10 mM BCH, MeAIB, and ACS, respectively. The results showed that both syn-3-[^18^F]FACBC and anti-2-[^18^F]FACBC are selective substrates for L-type amino acid transporters in L9 tumor cells in culture.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+rodentia)]

Ex vivo biodistribution studies of syn-3-[^18^F]FACBC were performed in rats (n = 4/group) implanted intracerebrally with 9L gliosarcoma (10). Accumulation of syn-3-[^18^F]FACBC in the tumors was 1.40 ± 0.49, 2.10 ± 0.96, 1.48 ± 0.09, and 1.93 ± 0.72% ID/g at 15, 30, 60, and 120 min after injection, respectively. The accumulation in the contralateral brain tissue and bone was ~0.18%–0.25% ID/g at these time points. Little defluorination was observed. The tissue with the highest accumulation at 30 min after injection was the pancreas (3.36% ID/g), followed by the kidney (0.80% ID/g), liver (0.60% ID/g), and lung (0.57% ID/g). The accumulation in other tissues (heart, spleen, muscle, and blood) was low (<0.5% ID/g). The tumor/brain ratios were 7.2, 11.5, 7.6, and 7.7 at 15, 30, 60, and 120 min, respectively. anti-3-[^18^F]FACBC and [^18^F]FDG exhibited tumor/brain ratios of 6.6 and 0.84, respectively, at 60 min in the same tumor model. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facbc%5BAll%20Fields%5D%20AND%20human)]

No publication is currently available.

## References

1 Coleman R.E., Hoffman J.M., Hanson M.W., Sostman H.D., Schold S.C. (1991). Clinical application of PET for the evaluation of brain tumors. J Nucl Med.
2 Kaschten B., Stevenaert A., Sadzot B., Deprez M., Degueldre C., Del Fiore G., Luxen A., Reznik M. (1998). Preoperative evaluation of 54 gliomas by PET with fluorine-18-fluorodeoxyglucose and/or carbon-11-methionine. J Nucl Med.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
5 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
6 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
7 Palacin M., Estevez R., Bertran J., Zorzano A. (1998). Molecular biology of mammalian plasma membrane amino acid transporters. Physiol Rev.
8 Shoup T.M., Olson J., Hoffman J.M., Votaw J., Eshima D., Eshima L., Camp V.M., Stabin M., Votaw D., Goodman M.M. (1999). Synthesis and evaluation of [18F]1-amino-3-fluorocyclobutane-1-carboxylic acid to image brain tumors. J Nucl Med.
9 Schuster D.M., Votaw J.R., Nieh P.T., Yu W., Nye J.A., Master V., Bowman F.D., Issa M.M., Goodman M.M. (2007). Initial experience with the radiotracer anti-1-amino-3-18F-fluorocyclobutane-1-carboxylic acid with PET/CT in prostate carcinoma. J Nucl Med.
10 Yu W., Williams L., Camp V.M., Malveaux E., Olson J.J., Goodman M.M. (2009). Stereoselective synthesis and biological evaluation of syn-1-amino-3-[18F]fluorocyclobutyl-1-carboxylic acid as a potential positron emission tomography brain tumor imaging agent. Bioorg Med Chem.